# ^99m^Tc-Labeled S-benzoylmercaptoacetyl triglycine N-acetylglucosamine

Chemical name: | ^99m^Tc-Labeled S-benzoylmercaptoacetyl triglycine N-acetylglucosamine
Abbreviated name: | [^99m^Tc]SBz-MAG_3_-NG
Synonym: | [^99m^Tc]MAG_3_-NG
Agent Category: | Compound
Target: | Lectins
Target Category: | Proteins
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure of [^99m^Tc]SBz-MAG_3_-NG. Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=lectins&cmd=DetailsSearch)]

Lectins are proteins that bind carbohydrates reversibly and are present on the membrane surface of all prokaryotic and eukaryotic cells. It is known that the carbohydrate–lectin interactions result in the initiation of a fight against or the development of a variety of conditions such as cancer metastases (1), pathological inflammation (2), and microbial infections (3). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=lectins) approved by the United States Food and Drug Administration are under way to evaluate the use of lectins to treat a variety of infections and cancerous tumors. Because of their role in the modulation of diverse physiological processes and diseases, investigators are increasingly interested in studying lectins for the development (4) and delivery of therapeutic drugs in humans (5). Although lectin glycoarrays have been used to profile different glycoproteins (6), no agents are presently available to investigate the function of the lectin-carbohydrate complexes under in vivo conditions. In an effort to develop imaging agents for the in vivo study of lectins, de Barros et al. (7) synthesized glucose (Gl), N-acetylglucosamine (NG), and galactose (Ga) respectively conjugated to S-benzoylmercaptoacetyl triglycine (SBz-MAG_3_) and labeled these compounds with ^99m^Tc to obtain [^99m^Tc]SBz-MAG_3_-NG (or [^99m^Tc]MAG_3_-NG), [^99m^Tc]SBz-MAG_3_-Gl (or [^99m^Tc]MAG_3_-Gl), and [^99m^Tc]SBz-MAG_3_-Ga (or [^99m^Tc]MAG_3_-Ga). The biodistribution of these radiolabeled carbohydrates was then studied in normal Swiss mice (7). This chapter describes the results obtained with [^99m^Tc]SBz-MAG_3_-NG. Results obtained with [^99m^Tc]SBz-MAG_3_-Gl (8) and [^99m^Tc]SBz-MAG_3_-Ga (9) are presented in separate chapters in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20synthesis&cmd=DetailsSearch)]

The synthesis of [^99m^Tc]SBz-MAG_3_-NG was described by de Barros et al. (7). The radiochemical purity of the tracer was reported to be >90%. The radiochemical yield, specific activity, and stability of [^99m^Tc]SBz-MAG_3_-NG were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20in%20Vitro%20studies&cmd=DetailsSearch)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]SBz-MAG_3_-NG was studied in normal Swiss mice (7). The animals (n = 5 mice per time point) were injected with the radiochemical, and the mice were euthanized at various time points from 5 to 60 min post-injection (p.i.) to collect all major organs and to determine the accumulated radioactivity. At 5 min p.i., maximum accumulation of label was in the bladder (33.92 ± 7.56% injected dose per gram tissue (% ID/g)), followed by the kidneys (16.81 ± 2.24% ID/g), liver (9.58 ± 0.81% ID/g), blood (7.33 ± 1.40% ID/g), and lungs (4.00 ± 0.64% ID/g). At 60 min p.i., the bladder had the highest amount of radioactivity (89.07 ± 5.01% ID/g), followed by kidneys (1.93 ± 0.41% ID/g), liver (1.88 ± 0.44% ID/g), blood (1.18 ± 0.24% ID/g), and lungs (0.67 ± 0.12% ID/g). This study indicated that radioactivity either as [^99m^Tc]SBz-MAG_3_-NG or as a metabolite was excreted primarily through the urinary route. The radioactivity uptake pattern with [^99m^Tc]SBz-MAG_3_-NG was similar to that observed with [^99m^Tc]SBz-MAG_3_-Gl (8) and [^99m^Tc]SBz-MAG_3_-Ga (9). However, accumulation of [^99m^Tc]SBz-MAG_3_-Ga was significantly (P < 0.05) higher in the liver at both 5 min and 60 min p.i. than that of either [^99m^Tc]SBz-MAG_3_-Gl (8.77 ± 1.22% ID/g at 5 min and 1.82 ± 0.15% ID/g at 60 min p.i.) or [^99m^Tc]SBz-MAG_3_-NG (9.58 ± 0.81% ID/g at 5 min and 1.88 ± 0.44% ID/g at 60 min p.i.). No blocking studies were reported.

From these studies, the investigators concluded that [^99m^Tc]SBz-MAG_3_-NG behaved in a manner similar to [^99m^Tc]SBz-MAG_3_-Gl when injected into mice (7). Among the three labeled compounds, only [^99m^Tc]SBz-MAG_3_-Ga was considered suitable as an imaging agent to evaluate hepatic function.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20non%20primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20non%20human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Makrilia N., Kollias A., Manolopoulos L., Syrigos K. (2009). Cell adhesion molecules: role and clinical significance in cancer. Cancer Invest.
2 Yang R.Y., Rabinovich G.A., Liu F.T. (2008). Galectins: structure, function and therapeutic potential. Expert Rev Mol Med.
3 Haagsman H.P., Hogenkamp A., van Eijk M., Veldhuizen E.J. (2008). Surfactant collectins and innate immunity. Neonatology.
4 Ernst B., Magnani J.L. (2009). From carbohydrate leads to glycomimetic drugs. Nat Rev Drug Discov.
5 Darbre T., Reymond J.L. (2008). Glycopeptide dendrimers for biomedical applications. Curr Top Med Chem.
6 Zhao J., Patwa T.H., Qiu W., Shedden K., Hinderer R., Misek D.E., Anderson M.A., Simeone D.M., Lubman D.M. (2007). Glycoprotein microarrays with multi-lectin detection: unique lectin binding patterns as a tool for classifying normal, chronic pancreatitis and pancreatic cancer sera. J Proteome Res.
7 de Barros, A.L., V.N. Cardoso, L.D. Mota, and R.J. Alves, Synthesis and biodistribution studies of carbohydrate derivatives radiolabeled with technetium-99m. Bioorg Med Chem Lett, 2009
8 Chopra, A., 99mTc-Labeled S-benzoylmercaptoacetyl triglycine D-glucose. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Chopra, A., 99mTc-Labeled S-benzoylmercaptoacetyl triglycine D-galactose. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.